# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_
Abbreviated name: | ^64^Cu-DOTA-NFB
Synonym: | ^64^Cu-DOTA-TN14003
Agent category: | Peptide
Target: | Chemokine receptor 4 (CXCR4)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB)]

Chemokine receptors are G-protein–coupled receptors directing cell movement toward higher concentrations of chemokines. Chemokine receptor 4 (CXCR4) and its ligand, stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and hematopoietic systems (1, 2). In addition, this CXCR4-SDF-1 receptor system has a function in the development, progression, and spread of various cancers (3), and CXCR4 acts as a co-receptor for human immunodeficiency virus (HIV) on CD4^+^ T cells (4). It has been suggested that CXCR4/SDF-1 interaction contributes to the pathogenesis of neurodegenerative and inflammatory conditions (5). CXCR4 is expressed by many different types of cancers, and overexpression of CXCR4 in cancers indicates poor prognosis with aggressive and metastatic tumors and resistance to chemotherapy (6).

CXCR4 is considered to play an important role in HIV infections and cancers. It is critical to perform imaging studies to measure CXCR4 levels under in vivo conditions for various pathological and physiological conditions (7). ^99m^Tc-SDF-1 has been used with single-photon emission computed tomography (SPECT) to determine changes in CXCR4 expression in the heart after a myocardial infarction. ^64^Cu-1,1'-[1,4-Phenylenebis(methylene)]-bis[1,4,8,11-tetraaza-cyclotetradecane] (^64^Cu-AMD3100), an inhibitor of CXCR4 activity, has been studied with positron emission tomography (PET) (8). An ^111^In-labeled CXCR4 antagonist peptide, ^111^In-Ac-TZ14011, has been developed for SPECT imaging of CXCR4 expression in xenograft tumors in mice (9). Tamamura et al. (10) identified TN14003, a 14-amino-acid peptide (Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_) with high anti-HIV and CXCR4 antagonistic activities in vitro. Jacobson et al. (11) radiolabeled TN14003 with 4-[^18^F]fluorobenzoic acid ([^18^F]FBA) to form 4-[^18^F]fluorobenzoyl-Arg-Arg-Natl-Cys-Tyr-Cit-Lys-D-Lys-Pro-Tyr-Arg-Cit-Cys-Arg-NH_2_ (4-[^18^F]F-T140 (http://www.ncbi.nlm.nih.gov/books/NBK53566/#T140-4-18F)) for PET imaging of tumor CXCR4 expression with a high tumor/background ratio. However, 4-[^18^F]F-T140 exhibited high nonspecific accumulation in red blood cells (RBCs), which masked its binding to CXCR4 on tumors. Later, Jacobson et al. (12) replaced 4-fluorobenzoyl in T140 with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-1,4,7,10-tetraacetic acid (DOTA) to form DOTA-NFB or 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA) to form NOTA-NFB for radiolabeling with ^64^Cu. ^64^Cu-DOTA-NFB and ^64^Cu-NOTA-NFB showed higher tumor/background ratios than 4-[^18^F]F-T140 with lower bindings to RBCs.

### Related Resource Links:

- Chapters in MICAD (CXCR4 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CXCR4+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (CXCR4 (http://www.ncbi.nlm.nih.gov/gene/7852))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CXCR4 (http://www.ncbi.nlm.nih.gov/omim/162643))
- Clinical trials (CXCR4 (http://www.clinicaltrials.gov/ct2/results?term=CXCR4))
- Drug information in FDA (CXCR4 (http://google2.fda.gov/search?q=CXCR4&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20synthesis)]

Jacobson et al. (12) incubated TN14003 (0.84 µmol) and DOTA-N-hydroxysuccinimide ester (1.01 µmol) in dimethylformamide and diisopropylethylamine for 18 h at 4°C. DOTA-NFB was obtained with 50%–62% chemical yield after purification with high-performance liquid chromatography (HPLC). The structure of DOTA-NFB was confirmed with HPLC and mass spectroscopy analysis supporting a 1:1 DOTA to NFB conjugation. Radiolabeling was performed by mixing 370–444 MBq (10–12 mCi) ^64^Cu-acetate with DOTA-NFB (12 nmol) in ammonium acetate buffer at pH 5.5. The mixture was heated for 20 min at 40°C. ^64^Cu-DOTA-NFB was purified with HPLC. The radiochemical purity was 99%, with a specific activity of 37 MBq/nmol (1 mCi/nmol) at the end of purification. The labeling yield was 91 ± 3% (n =5), with a total synthesis time of 50–55 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20in%20vitro)]

Chinese hamster ovary (CHO) cells were transfected with human CXCR4 (7 × 10^5^ binding sites/cell). A receptor-binding assay was performed with ^125^I-SDF-1. T140 exhibited a 50% inhibition concentration (IC_50_) value of 2.5 nM (11), whereas DOTA-NFB showed a IC_50_ value of 68 nM (12). T140 also exhibited a lower IC_50_ value than DOTA-NFB to inhibit Jurkat T cell migration in response to SDF-1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20rodentia)]

Jacobson et al. (12) performed ex vivo biodistribution studies of 1.85 MBq (0.05 mCi) ^64^Cu-DOTA-NFB in nude mice (n = 5) bearing CHO and CHO-CXCR4 tumor xenografts at 4 h after injection. Accumulation in the spleen (CXCR4-expressing organ) was 6.7 ± 0.8% injected dose/gram (ID/g). The blood accumulation was low at <0.5% ID/g. Accumulation in the liver (18% ID/g) and kidneys (60% ID/g) was higher than in the spleen. The accumulation of radioactivity was significantly higher (P > 0.05) in the CHO-CXCR4 tumors (5.0 ± 0.9% ID/g) than in the CXCR4-negative CHO tumors (~1% ID/g). Co-injection of excess DOTA-NFB (20 nmol) significantly reduced (P < 0.01) the accumulation of radioactivity in the spleen and CXCR4-positive tumors but had little effect in the blood, muscle, liver, and CHO tumors. On the other hand, the accumulation in the kidneys increased to ~80% ID/g. The tumor/blood and tumor/muscle ratios were 14.5 ± 0.8 and 19.3 ± 2.4, respectively, at 4 h after injection of only ^64^Cu-DOTA-NFB. Co-injection with 20 nmol DOTA-NFB significantly decreased the tumor/blood and tumor/muscle ratios to 3.8 ± 0.2 and 8.2 ± 2.7 (P < 0.01), respectively.

The whole-body distribution of ^64^Cu-DOTA-NFB was assessed with static PET imaging at 1, 2, 4, and 24 h after injection in nude mice (n = 5) bearing CHO and CHO-CXCR4 tumor xenografts (12). The CHO-CXCR4 tumors were clearly visualized along with the abdomen area at 1 h after injection, but the CHO tumors were not. The accumulation in the CHO-CXCR4 tumors was constant over time at ~4% ID/g. There was little radioactivity (<0.5% ID/g) in the blood and muscle. The liver and kidneys exhibited slow washout, with 13.6% ID/g and 22.4% ID/g at 24 h, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DOTA-NFB%20and%20human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
7 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
8 Jacobson O., Weiss I.D., Szajek L., Farber J.M., Kiesewetter D.O. (2009). 64Cu-AMD3100--a novel imaging agent for targeting chemokine receptor CXCR4. Bioorg Med Chem.
9 Hanaoka H., Mukai T., Tamamura H., Mori T., Ishino S., Ogawa K., Iida Y., Doi R., Fujii N., Saji H. (2006). Development of a 111In-labeled peptide derivative targeting a chemokine receptor, CXCR4, for imaging tumors. Nucl Med Biol.
10 Tamamura H., Xu Y., Hattori T., Zhang X., Arakaki R., Kanbara K., Omagari A., Otaka A., Ibuka T., Yamamoto N., Nakashima H., Fujii N. (1998). A low-molecular-weight inhibitor against the chemokine receptor CXCR4: a strong anti-HIV peptide T140. Biochem Biophys Res Commun.
11 Jacobson O., Weiss I.D., Kiesewetter D.O., Farber J.M., Chen X. (2010). PET of tumor CXCR4 expression with 4-18F-T140. J Nucl Med.
12 Jacobson, O., I.D. Weiss, L.P. Szajek, G. Niu, Y. Ma, D.O. Kiesewetter, A. Peled, H.S. Eden, J.M. Farber, and X. Chen, Improvement of CXCR4 tracer specificity for PET imaging. J Control Release, 2011